# [^11^C]Triphenylmethylphosphonium

Chemical name: | [^11^C]Triphenylmethylphosphonium
Abbreviated name: | [^11^C]TPMP
Synonym:
Agent category: | Compound
Target: | Mitochondria
Target category: | Lipophilic cation, membrane potential
Method of detection: | PET
Source of signal: | ^11^C
Activation:
Studies: | - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP)]

Lipophilic cations are capable to pass through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to a large negative plasma- and mitochondrial- membrane potentials. ^99m^Tc-2-methoxyisobutylisonitrile (^99m^Tc-MIBI (http://www.ncbi.nlm.nih.gov/books/NBK23098/)) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells being driven by metabolic demand and membrane potential (1-4). They are used as myocardial perfusion single photon emission computed tomography (SPECT) as well as tumor imaging agents. However, the high accumulation of technetium tracers in the lung and liver may hinder the detection of flow abnormalities in the myocardium.

Triphenylmethylphosphonium is a lipophilic cation and has been used to measure membrane potentials of cells in vitro (5). [^11^C]Triphenylmethylphosphonium ([^11^C]TPMP) has been investigated as a positron emission tomography (PET) agent for myocardial and tumor imaging to provide a better temporal and spatial resolution than SPECT.

### Related Resource Links:

- Chapters in MICAD (Lipophilic cation (http://www.ncbi.nlm.nih.gov/books/?term=lipophilic%20cation%20%20AND%20micad%5Bbook%5D))
- Clinical trials (^99m^Tc-MIBI (http://www.clinicaltrials.gov/ct2/results?term=99mTc+Sestamibi))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc++MIBI&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=0&y=0))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20synthesis)]

[^11^C]TPMP was prepared by reacting [^11^C]methyl iodide with triphenylphosphonium with a radiochemical yield of 9-13% (based on [^11^C]CO_2_) and specific activities of 15-33 GBq/μmol (400-900 mCi/μmol) at end of synthesis (6). The total synthesis time was 30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20rodentia)]

Biodistribution studies in rats injected with 0.037-0.111 MBq (1-3 µCi) [^14^C]TPMP were performed by Fukuda et al. (6) showing high accumulation of radioactivity in the heart (3.05 ± 0.16% injected dose (ID) at 2 min and 4.14 ± 0.83%ID at 60 min post injection. The bulk of accumulation was in the lungs, liver, intestine, and kidneys at 2 min. Clearance of radioactivity occurred at 60 min for all tissues except the heart. The heart/blood ratios were 31 at 2 min, 50 at 10 min, 93 at 30 min and 154 at 60 min. Ex vivo whole-body autoradiographic studies of rats at 30 and 120 min showed high radioactivity in the myocardium, small intestine and urinary bladder with little radioactivity in the heart cavity, brain and spinal cord.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Fukuda et al. (6) performed PET imaging measurements of [^11^C]TPMP binding in the heart of one dog injected intravenously with 666 MBq (18 mCi) of [^11^C]TPMP. PET scans showed distinct accumulation of [^11^C]TPMP in the myocardium. Within the time interval between 20 and 60 min after injection, the radioactivity retained in the heart was 0.045%ID/ml and 0.049%ID/ml, respectively. The heart/blood ratios were 40 at 20 min and 74 at 60 min.

Krause et al. (7) performed PET imaging in 4 mongrel dogs to study extraction fraction and uptake measurements of [^11^C]TPMP. Under normal flow conditions [^11^C]TPMP uptake reached a maximum within the first 10 min after injection and remained constant during the entire observation period of 80 min. Over the same time period, the heart/blood ratio was 46-106, and the heart/lung ratio 14. Following permanent occlusion of the left anterior descending coronary artery, [^11^C]TPMP uptake in the normally perfused myocardium also reached a maximum at 10 minutes after injection, whereas in the infarcted area there was no significant accumulation of [^11^C]TPMP. For a time period of 80 min the noninfarcted/infarcted myocardium ratio was 12. Extraction was measured in dogs with a double isotope method using ^99m^Tc-HSA as the reference tracer. The extraction fraction was 91% at a flow of 0.69 ml/min/g. As flow increased to five-fold (3.42 ml/min/g) following administration of adenosine, extraction fell to 61%. Following coronary artery occlusion, the [^11^C]TPMP content in the myocardium was highly correlated (r = 0.93, p < 0.01) with the microsphere determined regional myocardial blood flow.

Madar et al. (8) performed [^11^C]TPMP PET imaging in 3 mongrel dogs bearing glioma tumor cells in the brain. [^11^C]TPMP exhibited enhanced uptake and prolonged retention in canine brain glioma tumor cells within 20-95 min. ^68^Ga-EDTA exhibited an enhanced uptake and a gradual washout from the tumor tissue, indicating that the blood-brain barrier was not intact. The tumor/normal brain uptake ratio at 55 to 95 min after injection was 47.5 ± 17.6 for [^11^C]TPMP and 8.1 ± 1.9 for ^68^Ga-EDTA. Qualitative comparison with histological sections showed that [^11^C]TPMP enhanced uptake was restricted to the tumor area.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20TPMP%20and%20human)]

No relevant publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
4 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
5 Mitchell P., Moyle J. (1969). Estimation of membrane potential and pH difference across the cristae membrane of rat liver mitochondria. Eur J Biochem.
6 Fukuda H., Syrota A., Charbonneau P., Vallois J., Crouzel M., Prenant C., Sastre J., Crouzel C. (1986). Use of 11C-triphenylmethylphosphonium for the evaluation of membrane potential in the heart by positron-emission tomography. Eur J Nucl Med.
7 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
8 Madar I., Anderson J.H., Szabo Z., Scheffel U., Kao P.F., Ravert H.T., Dannals R.F. (1999). Enhanced uptake of [11C]TPMP in canine brain tumor: a PET study. J Nucl Med.